# ^15^N-Labeled 4-oxo-2,2,6,6-tetramethyl-piperidine-1-oxyl

Chemical name: | ^15^N-Labeled 4-oxo-2,2,6,6-tetramethyl-piperidine-1-oxyl
Abbreviated name: | [^15^N]TEMPONE
Synonym: | ^15^N-Labeled 2,2,6,6-tetramethyl-4-oxo-piperidine-1-oxyl, ^15^N-labeled 2,2,6,6-tetramethyl-4-oxo-piperidine-N-oxy free radical, ^15^N-labeled triacetoneamine-N-oxyl, ^15^N-labeled-4-oxo-TEMPONE
Agent catagory: | Small molecule
Target: | Other
Target category: | Other –reactive oxygen species (ROS)
Method of detection: | Electron paramagnetic resonance imaging (EPRI), magnetic resonance imaging (MRI), proton electron double resonance imaging (PEDRI), Overhauser-enhanced MRI (OMRI)
Source of signal/contrast: | Nitroxide
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TEMPO + radicals)]

Reactive oxygen species (ROS) are various free radicals generated in a biological milieu (1, 2). They are propagated through a cascade of reactions in the pathogenesis in many diseases, including cancer, stroke, atherosclerosis, ischemia-reperfusion injury, Alzheimer’s disease, diabetic vascular diseases, and inflammatory diseases (2). In particular, ROS interact with glutathione (GSH), NADPH, and ascorbates to maintain cellular redox status (3). Therefore, the distribution of ROS in tissue can be used as a surrogate marker to characterize the redox status/environment in disease-related physiological and pathological conditions (1). Because all free radicals contain unpaired electrons, the electron paramagnetic resonance (EPR) technique, also called electron spin resonance (ESR), is specific for detecting and quantifying ROS (2). EPR spectra can provide a wealth of information for unequivocal identification of free radicals, such as fine, hyperfine, and superhyperfine structures, g-factor, and lineshape (2). EPR imaging (EPRI) technique allows for non-invasive mapping of free radicals in animals/organs (4).

EPR is fundamentally similar to nuclear magnetic resonance (NMR) (5). However, the differences in the physical and chemical properties of the resonance species (unpaired electrons versus nuclear spin) lead to three major differences in acquiring the spectra/images: gyromagnetic ratio, relaxation time, and concentration (5). The gyromagnetic ratio of an electron spin is 658 times larger than that of a proton nuclear spin, resulting in a 658-fold increase in its magnetic moment and resonant frequency. For instance, with a magnet of 0.34 T, the EPR frequency of X-band is 9.5 GHz, and the NMR frequency of proton nuclei is 14.4 MHz. As a result of the presence of strong non-resonant water absorption, a high radiofrequency such as 9.5 GHz is not suitable for examining tissue samples. Thus, much lower EPR frequencies in the range of 1.2 GHz (L-band) to 300 MHz are used instead, corresponding to a penetration depth of a few cm. The increase in the magnetic moment of electron spin provides ~700 times greater intrinsic sensitivity with EPR on a molar basis than with NMR. Because the excited electron spins relax on a nanosecond time scale, which is several orders of magnitude shorter than the nuclear spin (measured in ms), pulsed EPR (Fourier transformation EPR (FT EPR) or time-domain EPR) is only applicable to those free radicals with an extremely narrow line, whereas most ERP spectrometers use the continuous wave technique (CW EPR). The lack of high concentrations of naturally occurring paramagnetic species such as free radicals often requires the addition of paramagnetic species. This in turn allows for the quantification of exogenous paramagnetic species but also requires the acquisition of the anatomic information with different imaging modalities such as magnetic resonance imaging (MRI). Proton electron double resonance imaging (PEDRI), also called Overhauser-enhanced magnetic resonance imaging (OMRI), is a double resonance technique that encodes characteristic EPR spectral information on a high-resolution MRI (6). This method uses EPR irradiation to saturate paramagnetic species and leads to polarization of water protons through the dynamic nuclear polarization (DNP) effect. The polarized protons produce enhanced signal intensity in MRI. PEDRI offers good sensitivity, high spatial resolution, and signal enhancement of approximately two orders of magnitude (7).

Nitroxides are stable organic free radicals that have a single unpaired electron delocalized between the nitrogen and the oxygen (8). The steric hindrance around the nitroxide group makes these compounds very stable. They can be obtained in pure form, and they can be stored and handled in the laboratory with no more precautions than most organic substances (9). Nitroxides used as the contrast agent in EPRI can detect the redox status on the basis of their reduction to EPR-silent hydroxylamine (10), and nitroxides have been extensively used in cells, tissues, and living animals (11). Inside cells, nitroxides are reduced to hydroxylamine by cellular antioxidants such as ascorbate, thioredoxin, reductase, ubiquinol, NADPH and GSH . Nitroxides also can function as superoxide dismutase mimics and repair DNA damage caused by ultraviolet irradiation. In addition to the use as an EPRI contrast agent, nitroxides are T_1_ relaxation agents in MRI for having an unpaired electron (12). Because their reduced form, hydroxylamine, is diamagnetic, the reduction process is accompanied by a decrease in T_1_ relaxivity. This decrease reflects the alterations in the redox status and can be used to map the redox status. Although the T_1_ relaxivity of nitroxides is much lower than that of gadolinium chelates (one unpaired electron versus seven unpaired electrons), their high cellular permeability leads to a significantly greater volume distribution in tissues and compensates for their lower relaxivity (12). Various nitroxides are designed to target different cellular compartments (8). For example, a neutral nitroxide can be distributed throughout the intracellular and extracellular environments, whereas a charged nitroxide is unable to cross the plasma membrane and can be used to measure oxygen levels in extracellular compartments.

^15^N-Labeled 4-oxo-2,2,6,6-tetramethyl-piperidine-1-oxyl ([^15^N]TEMPONE) is a ^15^N-labeled (spin = 1/2) neutral nitroxide (13). Commercially available TEMPONE exhibits low toxicity with a maximum tolerated dose (MTD) of ~1 mmol/kg (14). Compared to the commercial TEMPONE, which has a natural isotope of nitrogen (^14^N, spin = 1) with a triplet EPR hyperfine structure, [^15^N]TEMPONE has a doublet EPR hyperfine structure (13). The decrease in the number of hyperfine structures from three to two leads to a 1.5-fold increase in EPR signal intensity and DNP enhancement, assuming that the motional correlation time of hydroxides is faster than the inverse spin precession (Larmor) frequency of the electron spin (15). The characteristic doublet of ^15^N-labeled nitroxides is easily distinguished from the triplet structure in the natural isotope of ^14^N in other nitroxides. Thus, multiple nitroxides labeled with different isotopes (^14^N and ^15^N) can be used to separate different reduction or oxidation processes in vivo (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(15N labeled TEMPONE)+AND+synthesis%0D%0A)]

[^15^N]TEMPONE was synthesized by reaction of commercial phorone ((CH_3_)_2_CCHCOCHC((CH_3_)_2_) with ^15^N-labeled ammonium chloride (16).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(15N labeled TEMPONE)+AND+%22in+vitro%22)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(15N labeled TEMPONE) +AND++rodentia)]

Utsumi et al. examined the distribution of [^15^N]TEMPONE in mice (5 weeks old) in the presence of commercial ^14^N-nitroxides by OMRI (13). After intragastric administration of 200 μl of 10 mM [^15^N]TEMPONE followed by intravenous injection of 200 μl of 300 mM 3-carbamoyl-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxyl (3CP) solution, OMRI was conducted on a custom-built MRI spectrometer. The EPR excitation frequency values (B_0_^EPR^ ) for ^14^N-nitroxide and ^15^N-nitroxide were 6.103 mT and 6.563 mT, respectively, and the NMR frequency for proton nuclei was 617 kHz. Interleaved ESR excitation was used in the OMRI sequence to alternately excite the ^15^N-radicals ([^15^N]TEMPONE) and the ^14^N-enriched radicals (3CP). The images were collected at 1.5, 4.5, 7.5, and 11.5 min after the injection of 3CP. The signal of ^15^N-radicals appeared to be confined to the deposited site (i.e., the stomach), whereas the signal of ^14^N-radicals exhibited a global distribution over the whole mouse and their signal intensities were dependent on organ/region. This study demonstrated the possibility of tracking ^14^N- and ^15^N-labeled nitroxides simultaneously as well as the co-registration of their distribution in the same anatomic image.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(15N labeled TEMPONE) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(15N labeled TEMPONE) +AND+human)]

No publication is currently available.

### NIH Support

## References

1 Soule B.P., Hyodo F., Matsumoto K., Simone N.L., Cook J.A., Krishna M.C., Mitchell J.B. (2007). Therapeutic and clinical applications of nitroxide compounds. Antioxid Redox Signal.
2 Kuppusamy P., Zweier J.L. (2004). Cardiac applications of EPR imaging. NMR Biomed.
3 Hirayama A., Nagase S. (2006). Electron paramagnetic resonance imaging of oxidative stress in renal disease. Nephron Clin Pract.
4 Mikuni T., He G., Petryakov S., Fallouh M.M., Deng Y., Ishihara R., Kuppusamy P., Tatsuta M., Zweier J.L. (2004). In vivo detection of gastric cancer in rats by electron paramagnetic resonance imaging. Cancer Res.
5 Gallez B., Swartz H.M. (2004). In vivo EPR: when, how and why?. NMR Biomed.
6 Matsumoto K., Narazaki M., Ikehira H., Anzai K., Ikota N. (2007). Comparisons of EPR imaging and T1-weighted MRI for efficient imaging of nitroxyl contrast agents. J Magn Reson.
7 Hyodo F., Murugesan R., Matsumoto K., Hyodo E., Subramanian S., Mitchell J.B., Krishna M.C. (2008). Monitoring redox-sensitive paramagnetic contrast agent by EPRI, OMRI and MRI. J Magn Reson.
8 Gallez B., Baudelet C., Jordan B.F. (2004). Assessment of tumor oxygenation by electron paramagnetic resonance: principles and applications. NMR Biomed.
9 Holtzman, J.L., ed. Spin labeling in pharmacology1984, Academic Press, INC: New York. 5.
10 Kroll C., Borchert H.H. (1999). Metabolism of the stable nitroxyl radical 4-oxo-2,2,6, 6-tetramethylpiperidine-N-oxyl (TEMPONE). Eur J Pharm Sci.
11 Li H., He G., Deng Y., Kuppusamy P., Zweier J.L. (2006). In vivo proton electron double resonance imaging of the distribution and clearance of nitroxide radicals in mice. Magn Reson Med.
12 Hyodo F., Yasukawa K., Yamada K., Utsumi H. (2006). Spatially resolved time-course studies of free radical reactions with an EPRI/MRI fusion technique. Magn Reson Med.
13 Utsumi H., Yamada K., Ichikawa K., Sakai K., Kinoshita Y., Matsumoto S., Nagai M. (2006). Simultaneous molecular imaging of redox reactions monitored by Overhauser-enhanced MRI with 14N- and 15N-labeled nitroxyl radicals. Proc Natl Acad Sci U S A.
14 Matsumoto K., Krishna M.C., Mitchell J.B. (2004). Novel pharmacokinetic measurement using electron paramagnetic resonance spectroscopy and simulation of in vivo decay of various nitroxyl spin probes in mouse blood. J Pharmacol Exp Ther.
15 Swartz H.M., Khan N., Khramtsov V.V. (2007). Use of electron paramagnetic resonance spectroscopy to evaluate the redox state in vivo. Antioxid Redox Signal.
16 Jockusch S., Liu Z., Ottaviani M.F., Turro N.J. (2001). Time resolved CW-EPR spectroscopy of powdered samples: electron spin polarization of a nitroxyl radical adsorbed on NaY zeolite, generated by the quenching of excites triplet ketones. J. Phys. Chem. B.